# 6-Hydroxy-[1,1'-biphenyl]-3-yl-cyclohexyl-[^11^C-carbonyl]carbamate

Chemical name: | 6-Hydroxy-[1,1'-biphenyl]-3-yl-cyclohexyl-[^11^C-carbonyl]carbamate
Abbreviated name: | [^11^C]CURB
Synonym: | [^11^C-carbonyl]URB694, [^11^C]URB694
Agent category: | Compound
Target: | Fatty acid amide hydrolase (FAAH)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH)]

Fatty acid amide hydrolase (FAAH) is an integral membrane-bound serine hydrolase and a part of the endocannabinoid system (ECS), which comprises the cannabinoid receptors (CB1 and CB2), endogenous ligands termed endocannabinoids (anandamide and oleamide), transporters, and enzymes (1, 2). FAAH plays a key role in the hydrolysis of a number of primary and secondary fatty acid amides, controlling the levels of the neuromodulatory endocannabinoids in the ECS (3, 4). FAAH is widely expressed in many tissues, with the highest levels in the liver and brain (5). Genetic or pharmacological inactivation of FAAH in the brain leads to analgesic, anti-inflammatory, anxiolytic, and anti-depression effects in animal models (6-8).

Cyclohexylcarbamic acid 3'-carbamoylbiphenyl-3-yl ester (URB597) is an irreversible, substrate-like inhibitor of FAAH involving carbamylation of the catalytic nucleophilic Ser^241^ and the O-biaryl group as the leaving group (9-11). On the basis of the structure of URB597, Wyffels et al. (12) prepared biphenyl-3-yl-4-[^11^C]methoxyphenylcarbamate ([^11^C]-1) for in vivo positron emission tomography (PET) imaging studies of the brain FAAH in mice. It was proposed that the carbamylation of Ser^241^ would leave the [^11^C]-methoxyanilino group bound to the FAAH for visualization of FAAH in the brain. However, the results of in vitro and ex vivo studies indicated that [^11^C]-1 is a reversible inhibitor of FAAH, and the rapid brain washout of the tracer limits its utility as a PET agent for in vivo measurements of FAAH. Wilson et al. (13) reported the ^11^C-radiolabeling of a close analog of URB597, 6-hydroxy-[1,1'-biphenyl]-3-yl-cyclohexylcarbamate (URB694), yielding [^11^C-carbonyl]URB694 ([^11^C]CURB) for PET imaging of FAAH in the brain. [^11^C]CURB showed good brain accumulation with regional heterogeneity, irreversibility, and specific binding to FAAH in vivo in rats. Rusjan et al. (14) reported [^11^C]CURB PET studies in human brain.

### Related Resource Links:

- Chapters in MICAD (FAAH (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=FAAH+AND+micad%5Bbook%5D))
- Gene information in NCBI (FAAH (http://www.ncbi.nlm.nih.gov/gene/2166))
- Articles in Online Mendelian Inheritance in Man (OMIM) (FAAH (http://omim.org/entry/602935))
- Clinical trials (FAAH (http://www.clinicaltrials.gov/ct2/results?term=FAAH&Search=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20synthesis)]

Wilson et al. (13) synthesized [^11^C]CURB by reaction of [^11^C]CO_2_ with cyclohexylamine for 1 min at room temperature, followed by addition of 2-phenyl-1,4-dihydroquinone. [^11^C]CURB was purified with high-performance liquid chromatography. The specific activity of [^11^C]CURB was 80–160 GBq/μmol (2.2–4.4 Ci/µmol) at the time of injection. The radiochemical yield, radiochemical purity, and total synthesis time were not reported. The LogD_7.4_ value of [^11^C]CURB was 2.8 ± 0.1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20in%20vitro)]

Mor et al. (11) showed that unlabeled URB694 and URB597 inhibited the hydrolysis of [^3^H]-anandamide by FAAH with IC_50_ values of 30.0 ± 5.8 and 7.7 ± 1.5 nM, respectively. Both compounds were irreversibly bound to FAAH.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20rodentia)]

Ex vivo biodistribution studies in normal rats (n = 5/group) were performed at 5, 15, 40, and 60 min after intravenous injection of 50 MBq (1.35 mCi) [^11^C]CURB (13). The accumulation level of radioactivity was highest in the cortex, followed by the hippocampus, cerebellum, striatum, and hypothalamus, with standard uptake values of 1.5–2.5 at 5 min after injection. The distribution of radioactivity in the brain regions is in agreement with the known distribution of FAAH in the rat brain. The cortex/hypothalamus ratio was 2.8 at 60 min. Radioactivity in the blood was lower than in the brain. The brain/blood ratios increased from 5 at 5 min to 16 at 60 min after injection. Pretreatment (30 min) with various doses (10, 50, and 500 µg/kg) of URB594 inhibited the radioactivity in the brain in a dose-dependent manner at 60 min after injection of [^11^C]CURB. At the highest dose of URB594, radioactivity levels were reduced by 62%–86%, depending on the brain regions. Pretreatment with URB597 (2 mg/kg) reduced the radioactivity levels by 72%–88%. At 2 min, 18% of radioactivity was irreversibly bound to brain tissue increasing to 80% at 60 min. Pretreatment with excess URB597 almost completely abolished the tissue-binding radioactivity. [^11^C]CURB was 67%, 60%, 47%, and 45% intact in the plasma at 5, 15, 40, and 60 min, respectively, with two polar metabolites. On the other hand, 80% of radioactivity was bound to the brain tissue, and the soluble fraction contained 19% intact [^11^C]CURB and 1% metabolite at 40 min. The investigators concluded that [^11^C]CURB should be a useful tool as a PET agent for in vivo measurements of FAAH because of its good brain accumulation with regional heterogeneity, irreversibility, and specific binding to FAAH.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FAAH%20and%20human)]

Rusjan et al. (14) reported [^11^C]CURB PET studies in human brain using kinetic modeling in six healthy subjects (age 19-53 yr) scanned with arterial blood sampling for 90 min. [^11^C]CURB was 68%, 48%, and 37% intact in the plasma at 8, 20, and 90 min, respectively. High standard uptake values (SUVs) were observed in the putamen (4.3 ± 0.8), thalamus (4.2 ± 0.6), and anterior cingulate cortex (3.5 ± 0.5). Kinetic parameters were estimated regionally using a one-tissue compartment model (TCM), a 2-TCM, a 2-TCMi (with irreversible trapping), and an irreversible 3-TCM. The 2-TCMi provided the best identifiability of PET outcome measures among the models analyzed (coefficient of variation (COV) of the net influx constant K_i_ and the composite parameter λk_3_ (λ=K_1_/k_2_) <5%, and COV (k_3_) <10%). Binding of [^11^C]CURB in the healthy human brain can be well identified with an irreversible two-tissue compartment kinetic model using 60 minutes of scan data.

## References

1 Giang D.K., Cravatt B.F. (1997). Molecular characterization of human and mouse fatty acid amide hydrolases. Proc Natl Acad Sci U S A.
2 McKinney M.K., Cravatt B.F. (2005). Structure and function of fatty acid amide hydrolase. Annu Rev Biochem.
3 Bracey M.H., Hanson M.A., Masuda K.R., Stevens R.C., Cravatt B.F. (2002). Structural adaptations in a membrane enzyme that terminates endocannabinoid signaling. Science.
4 Egertova M., Giang D.K., Cravatt B.F., Elphick M.R. (1998). A new perspective on cannabinoid signalling: complementary localization of fatty acid amide hydrolase and the CB1 receptor in rat brain. Proc Biol Sci.
5 Thomas E.A., Cravatt B.F., Danielson P.E., Gilula N.B., Sutcliffe J.G. (1997). Fatty acid amide hydrolase, the degradative enzyme for anandamide and oleamide, has selective distribution in neurons within the rat central nervous system. J Neurosci Res.
6 Naidu P.S., Kinsey S.G., Guo T.L., Cravatt B.F., Lichtman A.H. (2010). Regulation of inflammatory pain by inhibition of fatty acid amide hydrolase. J Pharmacol Exp Ther.
7 Fowler C.J., Naidu P.S., Lichtman A., Onnis V. (2009). The case for the development of novel analgesic agents targeting both fatty acid amide hydrolase and either cyclooxygenase or TRPV1. Br J Pharmacol.
8 Bambico F.R., Duranti A., Tontini A., Tarzia G., Gobbi G. (2009). Endocannabinoids in the treatment of mood disorders: evidence from animal models. Curr Pharm Des.
9 Alexander J.P., Cravatt B.F. (2005). Mechanism of carbamate inactivation of FAAH: implications for the design of covalent inhibitors and in vivo functional probes for enzymes. Chem Biol.
10 Basso E., Duranti A., Mor M., Piomelli D., Tontini A., Tarzia G., Traldi P. (2004). Tandem mass spectrometric data-FAAH inhibitory activity relationships of some carbamic acid O-aryl esters. J Mass Spectrom.
11 Mor M., Rivara S., Lodola A., Plazzi P.V., Tarzia G., Duranti A., Tontini A., Piersanti G., Kathuria S., Piomelli D. (2004). Cyclohexylcarbamic acid 3'- or 4'-substituted biphenyl-3-yl esters as fatty acid amide hydrolase inhibitors: synthesis, quantitative structure-activity relationships, and molecular modeling studies. J Med Chem.
12 Wyffels L., Muccioli G.G., Kapanda C.N., Labar G., De Bruyne S., De Vos F., Lambert D.M. (2010). PET imaging of fatty acid amide hydrolase in the brain: synthesis and biological evaluation of an 11C-labelled URB597 analogue. Nucl Med Biol.
13 Wilson A.A., Garcia A., Parkes J., Houle S., Tong J., Vasdev N. (2011). [11C]CURB: Evaluation of a novel radiotracer for imaging fatty acid amide hydrolase by positron emission tomography. Nucl Med Biol.
14 Rusjan P.M., Wilson A.A., Mizrahi R., Boileau I., Chavez S.E., Lobaugh N.J., Kish S.J., Houle S., Tong J. (2013). Mapping human brain fatty acid amide hydrolase activity with PET. J Cereb Blood Flow Metab.